# (E)-3-(4-(Dimethylamino)phenyl)-1-(4-(2-(([^18^F]fluoroethoxy)ethoxy)ethoxy)phenyl)-2-propen-1-one

Chemical name: | (E)-3-(4-(Dimethylamino)phenyl)-1-(4-(2-(([^18^F]fluoroethoxy)ethoxy)ethoxy)phenyl)-2-propen-1-one
Abbreviated name: | [^18^F]7c
Synonym:
Agent category: | Compound
Target: | Aggregates of β-amyloid peptide
Target category: | Acceptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPEG%20chalcone)]

Alzheimer's disease (AD) is a form of dementia with gradual memory loss and progressive decline in mental functions (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of β-amyloid peptides consisting of 40–42 amino acids), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyperphosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-Amyloid peptides and the tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging, single-photon emission computed tomography, and positron emission tomography (PET) (8-13). The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human postmortem brain tissue and in transgenic mice. Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans and showed more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-Methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for the senile plaques in the brain (16). Ono et al. (17) reported the development of a series of fluorinated polyethylene glycol chalcones for PET imaging of β-amyloid plaques in the brain. One of them, (E)-3-(4-(dimethylamino)phenyl)-1-(4-(2-(([^18^F]fluoroethoxy)ethoxy)ethoxy)phenyl)-2-propen-1-one ([^18^F]7c), has been evaluated as a useful probe for detection of β-amyloid plaques in the brain.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Amyloid%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/104760)
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=amyloid))
- Drug information (Amyloid PET ligand (http://google2.fda.gov/search?q=amyloid+PET+ligand&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14)) in FDA

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPEG%20chalcone%20and%20synthesis)]

[^18^F]7c was readily synthesized by standard ^18^F-fluorination of the tosyl precursor with ([^18^F]KF/Kryptofix 2.2.2) (17). The radiochemical yield was 45% at the end of synthesis, and the specific activity was 35 GBq/μmol (0.95 Ci/μmol) at the end of synthesis. Radiochemical purity was >99% as determined with high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPEG%20chalcone%20and%20in%20vitro)]

Compound 7c exhibited a binding affinity (K_i_) of 38.9 ± 4.2 nM for aggregated β-amyloid (1-42) in competition with 4-dimethylamino-4’-[^125^I]iodo-chalcone ([^125^I]DMIC (17). The K_i_ value for DMIC was found to be 13.1 ± 3.0 nM. [^18^F]7c bound to the cortex of postmortem AD brain slices as visualized in autoradiography studies. [^18^F]7c was found to bind to Tg2576 transgenic mouse brain slices but not to normal brain slices. No blocking studies were carried out but control tissue was used.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20rodentia)]

[^18^F]7c (3.7 MBq, 100 μCi) was injected intravenously into normal mice (n = 4–5 mice/group) to study its accumulation in the brain at 2, 10, 30, and 60 min after injection (17). [^18^F]7c showed an initial rapid penetration into the brain with 3.48 ± 0.47% injected dose (ID)/g at 2 min and a quick washout (1.08% ID/g at 30 min). The radioactivity levels were 2.35% ID/g and 2.98% ID/g in the blood and bone at 30 min, respectively. The bone radioactivity increased to 3.58%ID/g at 60 min, suggesting defluorination.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BAY94-9172%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
17 Ono M., Watanabe R., Kawashima H., Cheng Y., Kimura H., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). Fluoro-pegylated chalcones as positron emission tomography probes for in vivo imaging of beta-amyloid plaques in Alzheimer's disease. J Med Chem.